# ^111^In-Labeled DTPA conjugated monoclonal antibody 12A8 that targets the c-kit receptor

Chemical name: | ^111^In-Labeled monoclonal antibody 12A8 that targets the c-kit receptor fragment
Abbreviated name: | [^111^In]12A8
Synonym:
Agent Category: | Antibody
Target: | Proto-oncogene c-Kit; tyrosine-protein kinase kit; Mast/stem cell growth factor receptor; CD117
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=c-kit&cmd=DetailsSearch)]

The c-kit (CD 117 antigen or stem cell factor ligand receptor) is a 145-kDa type III glycoprotein receptor tyrosine kinase (TK; encoded by the KIT proto-oncogene) that has a TK at the juxtamembrane position, which is activated when a ligand binds to the extracellular ligand-binding domain of the receptor (1). Almost 70% of gastrointestinal stromal tumors (GISTs) (http://www.cancer.gov/cancertopics/pdq/treatment/gist/HealthProfessional) are known to overexpress a c-kit that has a mutation in exon 11 and produces a constitutively activated TK that promotes the survival and proliferation of cells and leads to the development of a malignant phenotype in the cells of the GISTs (1, 2). The biology and mutations of the c-kit gene and the detection, diagnosis, and chemotherapy of the cancerous GISTs are discussed in detail elsewhere (3, 4). An immunohistochemical method is commonly used to detect the overexpression of c-kit in GIST cancers, but this invasive technique is known to generate variable results (3, 5). In addition, investigators often use positron emission tomography (PET) with ^18^F-fluoro-deoxyglucose to detect, monitor, and assess the response of GISTs to chemotherapy, but this radiolabeled probe does not distinguish between GISTs and other cancerous tumors that have an epithelial or lymphatic origin (6).

In an effort to develop a reliable method for the detection of GISTs, the ^111^In-labeled anti–c-kit monoclonal antibody (mAb) 12A8 ([^111^In]12A8) was developed and evaluated for the detection of xenograft GISTs in nude mice with the use of single-photon emission computed tomography (SPECT) (6). Recently, the Fab fragment of mAb 12A8 was labeled with ^111^In or with ^64^Cu to obtain [^111^In]12A8 Fab or [^64^Cu]12A8 Fab, and the two probes were evaluated for the detection of tumors that express c-kit in nude mice (2). This chapter describes the in vitro and in vivo studies performed with [^111^In]12A8. Investigations conducted with [^111^In]12A8 Fab and [^64^Cu]12A8 Fab are discussed in separate chapters of MICAD (www.micad.nih.gov) (7, 8).

### Other Sources of Information

c-kit–Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=c-kit+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human c-kit (also known as Hardy-Zuckerman 4 feline sarcoma viral oncogene-like protein (KIT)) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/HM015525.1) sequence (Source: NCBI GenBank)

Gene (http://www.ncbi.nlm.nih.gov/nuccore?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=3815) (human c-kit; Gene ID: 3815)

c-kit in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=c-kit)

Signaling events (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200175&source=NATURE&output-format=graphic&ppage=1&genes_a=3815) mediated by c-kit (Source: Pathways Interaction Database)

c-kit–Related clinical trials (http://clinicaltrials.gov/ct2/results?term=c-kit)

Information on c-kit in PubChem Bioassay (http://www.ncbi.nlm.nih.gov/pcassay/?term=c-kit)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20synthesis&cmd=DetailsSearch)]

Two clones of the c-kit mAb (12A8 and 41A11) were obtained from commercial sources and radioiodinated with ^125^I using the chloramine-T method as described by Sogawa et al. (6). The specific activities of the labeled mAbs ranged from 277.5 to 555.0 kBq/μg (7.5 to 15 μCi/μg). In addition, 12A8 was labeled with ^125^I using 3'-^125^I-iodohippuryl N-maleoyl-L-lysine (HML) to obtain [^125^I]HML-12A8. The radiochemical yield of purified [^125^I]HML-12A8 was ~37%, with a specific activity of ~11.8 kBq/μg (~0.32 μCi/μg).

The 12A8 and 41A11 mAbs were conjugated with N-[(R)-2-amino-3-(p-isothiocyanato-phenyl)propyl]-trans-(S,S)-cyclohexane-1,2-triaminepentaacetic acid (DTPA) and labeled with ^111^In to generate [^111^In]12A8 and [^111^In]41A11 as detailed elsewhere (6). The DTPA:mAb ratio and the specific activity of the two labeled mAbs were reported to be 2.5 and ~111 kBq/μg (3 μCi/μg), respectively.

For use as an isotype-matched control, a non-specific IgG was also labeled with ^125^I and ^111^In as described above (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20in%20vitro%20studies&cmd=DetailsSearch)]

All in vitro studies were performed with HEK293-c-kit-K642E cells (human embryonic kidney cells that were transfected with and stably express a mutated c-kit gene) (6). From cell-binding assays with [^125^I]12A8 IgG, [^125^I]HML-12A8 IgG, [^111^In]12A8 IgG, [^125^I]41A11 IgG, and [^111^In]41A11 IgG, it was determined that the immunoreactive fractions of these labeled mAbs were 90.8%, 83.6%, 86.3%, 86.4%, and 69.0%, respectively. Competitive binding assays showed that the dissociation constants of these mAbs for 2.4–7.9 × 10^4^ binding sites on the cells were 3.9 × 10^9^, 7.1 × 10^9^, 2.2 × 10^9^, 4.0 × 10^9^, and 3.1 × 10^9^ M−^1^, respectively. Cell internalization assays, in which the mAbs were labeled with ^125^I or ^111^In and incubated with the cells on ice for 1 h, revealed that ~80% of the label was associated with the cell membrane; however, 50% of the label was internalized by the cells and there was a steady decrease in the membrane-associated tracer when the incubation was performed for 3 h at 37°C. The investigators also observed that after 3 h at 37°C, only the cells incubated with [^125^I]12A8 IgG and [^125^I]HML-12A8 IgG lost internalized radioactivity and showed a simultaneous increase in the amount of label in the cell growth medium. After >21 h at 37°C, the amounts of internalized radioactivity in cells incubated with [^111^In]12A8 IgG , [^125^I]12A8 IgG, and [^125^I]HML-12A8 IgG were 81.1%, 60.4%, and 16.8%, respectively. Although the data were not presented in the publication, similar observations were reported for the labeled 41A11 mAb (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^125^I]12A8 IgG, [^125^I]HML-12A8 IgG, and [^111^In]12A8 IgG were studied in nude mice bearing HEK293-c-kit-K642E cell xenograft tumors as described by Sogawa et al. (6). The animals (n = 5 mice/group) were intravenously injected with 37 kBq (1 μCi) ^125^I- or ^111^In-labeled 12A8 IgG (protein concentration was adjusted to 5 μg/mouse by the addition of unlabeled 12A8) and euthanized at 24, 48, and 96 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the tumors and the major organs. All data were reported as percent of injected dose per gram tissue (% ID/g). The investigators observed similar biodistribution patterns in the tumor for the two radioiodinated 12A8 mAbs in the animals. With [^125^I]12A8 IgG , the maximum accumulation of radioactivity was 1.5 ± 0.6% ID/g at 24 h p.i. and decreased thereafter. The tumor/blood (T/B) ratios for [^125^I]12A8 IgG were low at all time points (0.2, 0.1, and 0.2 at 24, 48, and 96 h p.i., respectively), and the T/B ratios for [^125^I]HML-12A8 IgG were even lower. No blocking studies were reported.

With [^111^In]12A8 IgG , the accumulation of radioactivity in the tumors increased from 6.6 ± 2.0% ID/g at 24 h to 9.2 ± 3.5% ID/g at 96 h p.i., and during the same period the T/B ratio increased from 0.6 at 24 h to 1.3 at 96 h p.i (6). The uptake values of [^111^In]12A8 IgG in the liver, spleen, and kidney were higher than those of [^125^I]12A8 IgG in the same organs. In comparison, the tumor uptake of the non-specific ^111^In-labeled IgG remained between 2.9% ID/g and 3.3% ID/g from 24 h to 96 h p.i., and the T/B ratio was 0.1 at 96 h p.i. The biodistribution of [^111^In]12A8 IgG was also investigated in nude mice bearing GIST822 cell xenograft tumors (human GIST cells described by Tuveson et al. (9)) (6). At 96 h p.i., the tumor uptake of radioactivity was 5.3% ID/g with a T/B ratio of 0.9, and these values were lower than those observed with the HEK293-c-kit-K642E cell xenograft tumors at the same time point. From these results, the investigators concluded that the labeled mAb bound specifically to the c-kit expressed on the GIST tumor cells. No blocking studies were reported.

Gamma planar and SPECT images were acquired from mice bearing xenograft tumors derived from HEK293-c-kit-K642E cells (6). Planar imaging was performed on one anesthetized animal at 24, 48, and 96 h p.i. The tumor outline was first visible at 48 h p.i. and became clearly visible at 96 h p.i. SPECT images taken at 96 h p.i. showed that the tumor was clearly visible in the transverse, coronal, and saggital views of the animal. No blocking studies were reported.

From these studies, the investigators concluded that radioiodinated anti–c-kit mAbs were not suitable for the visualization of tumors that express c-kit in mice because the labeled mAbs were dehaloginated after internalization by the cells (6). However, the tumors positive for c-kit showed a high uptake of radioactivity when exposed to an ^111^In-labeled anti–c-kit mAb, and this radionuclide was suitable for the visualization of the tumors with SPECT imaging (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-12A8%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Aubin F., Blanke C.D. (2011). Metastatic gastrointestinal stromal tumors. Cancer Chemother Pharmacol.
2 Yoshida C., et al. (2011). Development of positron emission tomography probe of 64Cu-labeled anti-C-kit 12A8 Fab to measure protooncogene C-kit expression. Nucl Med Biol.
3 Corless C.L., Heinrich M.C. (2008). Molecular pathobiology of gastrointestinal stromal sarcomas. Annu Rev Pathol.
4 Wang W.L., et al. (2011). Mechanisms of resistance to imatinib and sunitinib in gastrointestinal stromal tumor. Cancer Chemother Pharmacol.
5 Miettinen M., Lasota J. (2005). KIT (CD117): a review on expression in normal and neoplastic tissues, and mutations and their clinicopathologic correlation. Appl Immunohistochem Mol Morphol.
6 Sogawa C., et al. (2010). C-kit-targeted imaging of gastrointestinal stromal tumor using radiolabeled anti-c-kit monoclonal antibody in a mouse tumor model. Nucl Med Biol.
7 Chopra, A., 111In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH2 (IMP-156). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 64Cu-Labeled anti-c-kit monoclonal antibody 12A8 Fab fragment. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Tuveson D.A., et al. (2001). STI571 inactivation of the gastrointestinal stromal tumor c-KIT oncoprotein: biological and clinical implications. Oncogene.